# ^111^In-Capromab pendetide

Chemical name: | ^111^In-Capromab pendetide
Abbreviated name: | ^111^In-CYT-356, ^111^In-GYK-DTPA-7E11-C5.3, ^111^In-DTPA-7E11-C5.3, ^111^In-7E11-C5.3
Synonym: | ProstaScint®
Agent Category: | Antibody
Target: | Prostate-specific membrane antigen (PSMA)
Target Category: | Antibody-antigen binding
Method of detection: | SPECT
Source of signal: | ^111^In
Activation: | No
Studies: | - In vitro; - Rodents; - Humans | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=4758398), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nucleotide&val=4758397) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=2346) for more information about PSMA.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28Capromab%20Pendetide%20or%20cyt-356%20or%207e11%29%20and%20Indium)]

Prostate-specific membrane antigen (PSMA) is a unique type II, transmembrane-bound glycoprotein that is overexpressed on prostate tumor cells and in the neovasculature of most of the solid tumors, but not in the vasculature of normal tissues (1, 2). This unique expression of PSMA makes it an important biomarker as well as a large extracellular target of imaging agents (3, 4). 7E11-C5, a monoclonal antibody against the cytoplasmic domain of PSMA, was found to be specific to prostate tumor tissues in humans when conjugated with glycyl-tyrosyl-(N-ε-diethylenetriamine pentacetic acid)-lysine (GYK-DTPA). Tumors often contain dying or necrotic cells with permeable membranes, allowing the binding of antibodies to the intracellular epitope of PSMA. The antibody conjugate (Capromab pendetide or CYT-365) was radiolabeled with ^111^Indium. ^111^In-CYT-356 was approved by the US Food and Drug Administration in 1996 for the detection of prostate carcinoma and soft tissue metastases in prostate cancer patients. Newer antibodies against the extracellular domain of PSMA are being developed for immunotherapy of prostate cancer (5, 6).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28Capromab%20Pendetide%20or%20cyt-356%20or%207e11%29%20and%20Indium%20and%20synthesis)]

Purified monoclonal antibody 7E11-C5.3 was coupled with GYK-DTPA by site-specifically generated reactive aldehyde groups on the oligosaccharides found on the heavy chain of the antibody (7). A mixture of ^111^InCl_3_ (37 MBq, 1 mCi) and the conjugated antibody (100 μg) was incubated for 1 h at 37ºC. ^111^In-CYT-356 was purified by high performance chromatography (8). The specific activity was 55.5-210.9 MBq/mg (1.5-5.7 mCi/mg).

^111^In-CYT-356 can be easily prepared from a commercially available kit consisting of two vials to be mixed: 1) a sterile solution of 185 MBq/ml (5 mCi/ml) ^111^In-choride in sodium acetate buffer; and 2) a sterile solution of 0.5 mg of CYT-356. The mixture was incubated at room temperature for 30 min and filtered through a 0.22-μm filter.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28Capromab%20Pendetide%20or%20cyt-356%20or%207e11%29%20and%20Indium%20and%20in%20vitro)]

LNCaP human prostate cancer cells were reported to have a K_d_ of 6.69 nM with [^131^I]7E11-C5 and B_max_ of 95,000 sites/cell in saturation binding studies (9) using intact cells. The binding was accounted for by a subpopulation of permeated cells produced when the cells were trypsinized and washed. Little internalization of the tracer was found over a period of 48 h at 37ºC. When permeated cells were used, the number of binding sites/cell was similar to [^131^I]J591, an antibody against the extracellular domain of PSMA. Using nonpermeated cells, [^131^I]J591 has a K_d_ of 1.83 nM and a B_max_ of 600,000-800,000 sites/cell.

Various immunohistochemical studies indicate that 7E11-C5 reacts weakly with normal prostate epithelial cells and strongly with malignant prostate epithelial cells but does not react with non-prostate tumors or most normal tissues (8, 10-14). It also stains endothelial cells in solid tumors, such as lung, renal, colon, and breast carcinomas but not in normal vascular endothelial cells (15, 16).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28Capromab%20Pendetide%20or%20cyt-356%20or%207e11%29%20and%20Indium%20and%20rodentia)]

Biodistribution of ^111^In-CYT-356 was studied in LNCaP tumor-bearing nude mice by ex vivo tissue radioactivity measurements (8). ^111^In-CYT-356 uptake in tumor was high with 14% injected dose/g (ID/g) on day 1 after injection of 11.7 μg of the tracer (0.59 MBq, 16 μCi). It increased to 30% ID/g on days 3 and 7. Tumor image was visible by scintigraphic scan on day 4. Uptake in the lung, spleen, liver, and kidney was 4-6% ID/g, whereas the muscle showed an uptake of <1% ID/g. Uptake in non-tumor organs was similar in tumor-bearing mice and normal mice. ^111^In-CYT-356 did not accumulate in PC-3 and Du-145 prostate tumor lines (PSMA negative). Furthermore, ^111^In-labeled GYK-DTPA-conjugated, nonspecific antibody did not localize to the LNCaP tumor.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28Capromab%20Pendetide%20or%20cyt-356%20or%207e11%29%20and%20Indium%20and%20%28dog%20or%20pig%20or%20rabbit%20or%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28Capromab%20Pendetide%20or%20cyt-356%20or%207e11%29%20and%20Indium%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28Capromab%20Pendetide%20or%20cyt-356%20or%207e11%29%20and%20Indium%20and%20human)]

Human dosimetry of ^111^In-CYT-356 was estimated in 25 prostate cancer patients (17). Dynamic whole-body positron emission tomography (PET) scans were acquired after the injection of 185 MBq (5 mCi) of ^111^In-CYT-356 over a 7-10-day period. The organ that received the highest absorbed dose was the liver (1.0 mGy/MBq or 3.7 rad/mCi), followed by the spleen (0.88 mGy/MBq or 3.3 rad/mCi), and the kidneys (0.67 mGy/MBq or 2.5 rad/mCi). The prostate was estimated at 0.44 mGy/MBq (1.63 rad/mCi). The effective dose was calculated as 0.25-0.29 mSv/MBq (0.93-1.07 rem/mCi).

In one of the pivotal studies, ^111^In-CYT-356 scans (152 patients with prostate cancer) had a sensitivity, specificity, and overall accuracy of 62, 72, and 68%, respectively (18). The sensitivity of computed tomography (CT) and magnetic resonance imaging (MRI) was 4% and 15%, respectively.

Sodee et al. (19) reported the results of a retrospective study of 2,290 ^111^In-CYT-356 scans of 2,154 patients with prostate cancer performed at 15 institutions. ^111^In-CYT-356 scans identified positive uptake in the prostate or fossa (70.4%), pelvic nodes (31.5%), pelvic and extrapelvic nodes (23.9%), and extrapelvic nodes only (11.0%). In patients with newly diagnosed prostate cancer (n = 487), there was a significant correlation (p < 0.001) of prostate-specific antigen (PSA) level with positive ^111^In-CYT-356 scans in the prostate bed and pelvic metastases. The association between PSA level and positive ^111^In-CYT-356 scans in the fossa recurrence was weaker (p < 0.033) in patients after surgery (n = 1,225) and was not significant for pelvic and extrapelvic metastases. There was no association between PSA level and ^111^In-CYT-356 scans in patients with radiation therapy (n = 340) or hormonal therapy (n = 238).

^111^In-CYT-356 imaging has been studied in the detection of nodal metastases, detection of recurrent prostate cancer, detection of occult extraprostatic fossa, and evaluation before definitive therapy in patients with prostate cancer [PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28Capromab%20Pendetide%20or%20cyt-356%20or%207e11%29%20and%20Indium%20and%20human%20and%20review)]. Fusion studies of ^111^In-CYT-356 scans with CT or MRI improve the prediction of lymph node metastases in patients for definitive local therapy (20, 21).

## References

1 Feneley M.R., Jan H., Granowska M., Mather S.J., Ellison D., Glass J., Coptcoat M., Kirby R.S., Ogden C., Oliver R.T., Badenoch D.F., Chinegwundoh F.I., Nargund V.H., Paris A.M., Britton K.E. (2000). Imaging with prostate-specific membrane antigen (PSMA) in prostate cancer. Prostate Cancer Prostatic Dis.
2 Ghosh A., Heston W.D. (2004). Tumor target prostate specific membrane antigen (PSMA) and its regulation in prostate cancer. J Cell Biochem.
3 Nanus D.M., Milowsky M.I., Kostakoglu L., Smith-Jones P.M., Vallabahajosula S., Goldsmith S.J., Bander N.H. (2003). Clinical use of monoclonal antibody HuJ591 therapy: targeting prostate specific membrane antigen. J Urol.
4 Nargund V., Al Hashmi D., Kumar P., Gordon S., Otitie U., Ellison D., Carroll M., Baithun S., Britton K.E. (2005). Imaging with radiolabelled monoclonal antibody (MUJ591) to prostate-specific membrane antigen in staging of clinically localized prostatic carcinoma: comparison with clinical, surgical and histological staging. BJU Int.
5 Bander N.H., Trabulsi E.J., Kostakoglu L., Yao D., Vallabhajosula S., Smith-Jones P., Joyce M.A., Milowsky M., Nanus D.M., Goldsmith S.J. (2003). Targeting metastatic prostate cancer with radiolabeled monoclonal antibody J591 to the extracellular domain of prostate specific membrane antigen. J Urol.
6 Smith-Jones P.M., Vallabhajosula S., Navarro V., Bastidas D., Goldsmith S.J., Bander N.H. (2003). Radiolabeled monoclonal antibodies specific to the extracellular domain of prostate-specific membrane antigen: preclinical studies in nude mice bearing LNCaP human prostate tumor. J Nucl Med.
7 Rodwell J.D., Alvarez V.L., Lee C., Lopes A.D., Goers J.W., King H.D., Powsner H.J., McKearn T.J. (1986). Site-specific covalent modification of monoclonal antibodies: in vitro and in vivo evaluations. Proc Natl Acad Sci U S A.
8 Lopes A.D., Davis W.L., Rosenstraus M.J., Uveges A.J., Gilman S.C. (1990). Immunohistochemical and pharmacokinetic characterization of the site-specific immunoconjugate CYT-356 derived from antiprostate monoclonal antibody 7E11-C5. Cancer Res.
9 Smith-Jones P.M., Vallabahajosula S., Goldsmith S.J., Navarro V., Hunter C.J., Bastidas D., Bander N.H. (2000). In vitro characterization of radiolabeled monoclonal antibodies specific for the extracellular domain of prostate-specific membrane antigen. Cancer Res.
10 Horoszewicz J.S., Kawinski E., Murphy G.P. (1987). Monoclonal antibodies to a new antigenic marker in epithelial prostatic cells and serum of prostatic cancer patients. Anticancer Res.
11 Murphy G.P., Elgamal A.A., Troychak M.J., Kenny G.M. (2000). Follow-up ProstaScint scans verify detection of occult soft-tissue recurrence after failure of primary prostate cancer therapy. Prostate.
12 Silver D.A., Pellicer I., Fair W.R., Heston W.D., Cordon-Cardo C. (1997). Prostate-specific membrane antigen expression in normal and malignant human tissues. Clin Cancer Res.
13 Sweat S.D., Pacelli A., Murphy G.P., Bostwick D.G. (1998). Prostate-specific membrane antigen expression is greatest in prostate adenocarcinoma and lymph node metastases. Urology.
14 Troyer J.K., Beckett M.L., Wright G.L. (1995). Detection and characterization of the prostate-specific membrane antigen (PSMA) in tissue extracts and body fluids. Int J Cancer.
15 Liu H., Moy P., Kim S., Xia Y., Rajasekaran A., Navarro V., Knudsen B., Bander N.H. (1997). Monoclonal antibodies to the extracellular domain of prostate-specific membrane antigen also react with tumor vascular endothelium. Cancer Res.
16 Chang S.S., O'Keefe D.S., Bacich D.J., Reuter V.E., Heston W.D., Gaudin P.B. (1999). Prostate-specific membrane antigen is produced in tumor-associated neovasculature. Clin Cancer Res.
17 Mardirossian G., Brill A.B., Dwyer K.M., Kahn D., Nelp W. (1996). Radiation absorbed dose from indium-111-CYT-356. J Nucl Med.
18 Manyak M.J., Hinkle G.H., Olsen J.O., Chiaccherini R.P., Partin A.W., Piantadosi S., Burgers J.K., Texter J.H., Neal C.E., Libertino J.A., Wright G.L., Maguire R.T. (1999). Immunoscintigraphy with indium-111-capromab pendetide: evaluation before definitive therapy in patients with prostate cancer. Urology.
19 Sodee D.B., Malguria N., Faulhaber P., Resnick M.I., Albert J., Bakale G. (2000). Multicenter ProstaScint imaging findings in 2154 patients with prostate cancer. The ProstaScint Imaging Centers. Urology.
20 Schettino C.J., Kramer E.L., Noz M.E., Taneja S., Padmanabhan P., Lepor H. (2004). Impact of fusion of indium-111 capromab pendetide volume data sets with those from MRI or CT in patients with recurrent prostate cancer. AJR Am J Roentgenol.
21 Wong T.Z., Turkington T.G., Polascik T.J., Coleman R.E. (2005). ProstaScint (capromab pendetide) imaging using hybrid gamma camera-CT technology. AJR Am J Roentgenol.